# ^18^F-Labeled N-(4-fluorobenzylidene)oxime-VENK[homoC]NKEMRNRYWEAALDPNLNNQQKRAKIRSIYDDP[homoC]-NH_2_ with a disulfide bridge between the two homoC

Chemical name: | ^18^F-Labeled N-(4-fluorobenzylidene)oxime-VENK[homoC]NKEMRNRYWEAALDPNLNNQQKRAKIRSIYDDP[homoC]-NH_2_ with a disulfide bridge between the two homoC
Abbreviated name: | ^18^F-FBO-MUT-DS
Synonym:
Agent Category: | Affibody, antibody
Target: | HER2
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=affibody%20and%20HER2%20and%20molecular%20imaging)]

The ^18^F-labeled N-(4-fluorobenzylidene)oxime (FBO)-VENK[homoC]NKEMRNRYWEAALDPNLNNQQKRAKIRSIYDDP[homoC]-NH_2_ (MUT-DS) conjugate with a disulfide bridge between the two homocysteines, abbreviated as ^18^F-FBO-MUT-DS, is a 2-helix affibody derivative that was synthesized by Miao et al. for positron emission tomography (PET) of HER2-expressing tumors (1).

Affibody molecules are a group of nonimmunogenic scaffold proteins that are derived from the B-domain of staphylococcal surface protein A (2, 3). These molecules have only 58 amino acid residues (~7 kDa), which form a 3-α-helical bundle structure (3, 4). Helices 1 and 2 bundles are responsible for the high binding affinity and specificity of affibodies to their targets, while helix 3 contributes to the affibody stabilization and is not involved in receptor recognition (4). Studies have further confirmed that the binding domain in the helices 1 and 2 bundles includes 13 amino acid residues that are surface-exposed (2). Therefore, large affibody libraries have been constructed by randomization of the 13 amino acid residues, and a large set of affibody molecules against a wide variety of targets have been selected from those libraries. Of them, the affibodies specific to HER2, including Z_HER2:342_ and Z_HER2:477_, have been intensively investigated in recent years (3, 5). These molecules have been radiolabeled and tested for molecular imaging of HER2-expressing tumors.

The investigators at Stanford University first tested the feasibility of the monomeric (~7 kDa) and dimeric (~14 kDa) forms of affibody Z_HER2:477_ for molecular imaging (6, 7). Both forms have been labeled with various radiouclides through chelating agents. Studies have shown that smaller affibody constructs perform better in vivo in terms of tumor uptake and clearance, which prompts them to generate smaller proteins with only α-helices 1 and 2 bundles (~4 kDa) (4, 6, 7). However, simple deletion of the helix 3 leads to significantly decreased binding affinity of the proteins because of decreased helix conformation (4). The investigators then applied various strategies to improve the helix conformation of the affibody molecules, including sequence mutation, placement of disulfide bridges, and inclusion of helix-promoting amino acids (4). Although the helix conformation (~15%, the amount of α-helix represented in the secondary structure of the affibodies) of the 2-helix molecules is still much lower than that of the parent 3-helix affibodies, the investigators successfully obtained a class of 2-helix small proteins with HER2-binding affinity up to 5 nM with these strategies (1, 8, 9). One of these 2-helix proteins is MUT-DS, which has α-helices 1 and 2 bundles with a disulfide bridge being formed between the two inserted homocysteines (4). The radiolabeled MUT-DS derivatives exhibited favorable pharmacokinetics for imaging HER2-expressing tumors. ^68^Ga-DOTA-MUT-DS, ^64^Cu-DOTA-MUT-DS, ^111^In-DOTA-MUT-DS, and ^18^F-FBO-MUT-DS are examples of the MUT-DS derivatives (1, 8, 9).

This chapter summarizes the data obtained with ^18^F-FBO-MUT-DS (1).

### Related Resource Links:

- Anti-HER2 affibody conjugates in MICAD:

^68^Ga-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK48901/), ^111^In-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK23176/), Alexa750-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK45127/), ^111^In-benzyl-DOTA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23058/), ^111^In-benzyl-DTPA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23322/), Eaff800 (http://www.ncbi.nlm.nih.gov/books/NBK45665/), DY-682-ABD-Z_HER2:342_ (Haff682) (http://www.ncbi.nlm.nih.gov/books/NBK45664/), ^99m^Tc-Z_2395_-C (http://www.ncbi.nlm.nih.gov/books/NBK23590/), [^111^In]-ABY-025 (http://www.ncbi.nlm.nih.gov/books/NBK45623/), ^111^In-BZ-DTPA-Z_EGFR:1907_ (http://www.ncbi.nlm.nih.gov/books/NBK23654/).

- HER2-related clinical trials for imaging and therapy (http://clinicaltrials.gov/ct2/results?term=HER2)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21761266)]

The linear aminooxy-functionalized (AO)-MUT-DS was synthesized with standard solid-phase peptide synthesis (purity, >95%) (1). Cyclization of the linear peptides was achieved with I_2_ oxidation of the two L-homocysteines to form a disulfide bridge. The measured molecular weight (MW) of AO-MUT-DS was 4,823.9 (calculated 4,823.4). The AO-MUT-DS was then reacted with 4-fluorobenzaldehyde to prepare nonradioactive FBO-MUT-DS as a standard compound. Recovery yield was 70%–90%, and no starting cyclized peptide was detected. The measured MW (4,926.9) of the purified FBO-MUT-DS was consistent with the expected MW (4,928.4).

^18^F-FBO-MUT-DS was prepared by conjugating 4-^18^F-fluorobenzaldehyde with AO-MUT-DS (1). The purity was >95%. The overall yield ranged from 13% to 18% (non-decay-corrected) and the specific activities were 20–32 MBq/nmol (0.54–0.86 mCi/nmol) at the end of synthesis. The total time needed for the radiosynthesis was ~100 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21761266)]

The binding affinities of AO-MUT-DS and FBO-MUT-DS with the extracellular domain of HER2 antigen were measured in vitro with surface plasmon resonance detection (1). The binding affinity of FBO-MUT-DS was slightly higher than that of AO-MUT-DS (2 nM and 1 nM, respectively). The off-rate of FBO-MUT-DS was found to be similar as the AO-MUT-DS with a dissociation constant of 7 × 10−^4^ 1/s. The on-rate of FBO-MUT-DS was only approximately one-fold higher than that of AO-MUT-DS, with association constants of 7.5 × 10^6^ 1 M/s (association time, >2 min).

The HER2-targeting ability for cultured cells was evaluated with SKOV3 human ovarian cancer cells over 1 h incubation with ^18^F-FBO-MUT-DS (1). ^18^F-FBO-MUT-DS quickly accumulated in SKOV3 cells and reached a value of 14% of applied activity at 0.25 h. The uptake was maintained at almost the same level until 1 h. When the probe was co-incubated with a large excess (final concentration 4 µg/ml) of nonradioactive Z_HER2:342_, the probe uptake dropped to only ~5% of applied activity after 0.25 h incubation at 37°C (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21761266)]

The biodistribution of ^18^F-FBO-MUT-DS was examined with mice bearing SKOV3 human ovarian tumors (n = 3 mice/time point) after tail vein injection of ^18^F-FBO-MUT-DS (1.11–1.85 MBq (30–50 μCi)) (1). Mice were euthanized at 1 h and 3 h after injection. ^18^F-FBO-MUT-DS showed rapid and high accumulation in the tumors (6.9 ± 3.8% of injected dose per gram of tissue (ID/g) at 1 h). ^18^F-FBO-MUT-DS also displayed relatively rapid blood clearance (2.4 ± 0.8% ID/g) at 1 h. Both renal and liver uptake values were ~7% ID/g at 1 h, which suggested that ^18^F-FBO-MUT-DS was cleared through the hepatobiliary and renal systems. Distribution at 3 h after injection was not described in detail. Co-injection of ^18^F-FBO-MUT-DS (1.11–1.85 MBq (30–50 μCi), 0.3 µg) and blocking agent Z_HER2:342_ (500 µg)blocked the tumor uptake of ^18^F-FBO-MUT-DS (1.8 ± 1.1% ID/g at 1 h after injection) (n = 3 mice).

The tumor targeting and imaging abilities were further confirmed with PET imaging in mice bearing SKOV3 tumors (n = 3) (1). Good tumor imaging contrast was observed at 1 h and 2 h after injection of ^18^F-FBO-MUT-DS. The washout rate of the probe from tumors was slow. After 3 h, high tumor accumulation could still be seen in the PET images, while the uptake values for normal organs such as the liver and kidney declined dramatically. There was no significant difference for the tumor uptake at 1 h and 2 h after injection (P > 0.05), but the difference was significant for the liver uptakes (P < 0.05). These results suggest the good tumor retention and fast normal organ clearance of the ^18^F-FBO-MUT-DS.

The in vivo metabolic stability of ^18^F-FBO-MUT-DS was analyzed at 1 h after tail vein injection of ^18^F-FBO-MUT-DS into the mice bearing SKOV3 tumors (1). Studies showed that 80% of the probe remained intact in tumor, but only a small percentage of the intact probe was observed from urine samples, indicating relatively rapid degradation of the probe to more polar molecules cleared from the blood by the kidney–urinary system. The result also showed that a small fraction of the probe was metabolized to a more lipophilic fragment in liver.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are available.

## References

1 Miao Z., Ren G., Jiang L., Liu H., Webster J.M., Zhang R., Namavari M., Gambhir S.S., Syud F., Cheng Z. (2011). A novel (18)F-labeled two-helix scaffold protein for PET imaging of HER2-positive tumor. Eur J Nucl Med Mol Imaging.
2 Friedman M., Nordberg E., Hoiden-Guthenberg I., Brismar H., Adams G.P., Nilsson F.Y., Carlsson J., Stahl S. (2007). Phage display selection of Affibody molecules with specific binding to the extracellular domain of the epidermal growth factor receptor. Protein Eng Des Sel.
3 Orlova A., Feldwisch J., Abrahmsen L., Tolmachev V. (2007). Update: affibody molecules for molecular imaging and therapy for cancer. Cancer Biother Radiopharm.
4 Webster J.M., Zhang R., Gambhir S.S., Cheng Z., Syud F.A. (2009). Engineered two-helix small proteins for molecular recognition. Chembiochem.
5 Gao J., Chen K., Miao Z., Ren G., Chen X., Gambhir S.S., Cheng Z. (2011). Affibody-based nanoprobes for HER2-expressing cell and tumor imaging. Biomaterials.
6 Cheng Z., De Jesus O.P., Kramer D.J., De A., Webster J.M., Gheysens O., Levi J., Namavari M., Wang S., Park J.M., Zhang R., Liu H., Lee B., Syud F.A., Gambhir S.S. (2010). 64Cu-labeled affibody molecules for imaging of HER2 expressing tumors. Mol Imaging Biol.
7 Cheng Z., De Jesus O.P., Namavari M., De A., Levi J., Webster J.M., Zhang R., Lee B., Syud F.A., Gambhir S.S. (2008). Small-animal PET imaging of human epidermal growth factor receptor type 2 expression with site-specific 18F-labeled protein scaffold molecules. J Nucl Med.
8 Ren, G., J.M. Webster, Z. Liu, R. Zhang, Z. Miao, H. Liu, S.S. Gambhir, F.A. Syud, and Z. Cheng, In vivo targeting of HER2-positive tumor using 2-helix affibody molecules. Amino Acids, 2011
9 Ren G., Zhang R., Liu Z., Webster J.M., Miao Z., Gambhir S.S., Syud F.A., Cheng Z. (2009). A 2-helix small protein labeled with 68Ga for PET imaging of HER2 expression. J Nucl Med.